# Bimodal lentiviral vector encoding myc-tagged human ferritin heavy chain and green fluorescent protein (GFP)

Chemical name: | Bimodal lentiviral vector encoding myc-tagged human ferritin heavy chain and green fluorescent protein (GFP) | [image]
Abbreviated name: | Lenti-myc-hFTH | [image]
Synonym: | Myc-hFTH | [image]
Agent Category: | Viruses | [image]
Target: | Cells | [image]
Target Category: | Others (cell tracking) | [image]
Method of detection: | Multimodality (magnetic resonance imaging and optical imaging) | [image]
Source of signal / contrast: | Iron and GFP | [image]
Activation: | Yes | [image]
Studies: | - In vitro; - Rodents | Schematic diagram of the lentiviral vector (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=ferritin+and+MRI+and+reporter+gene)]

The bimodal lentiviral vector encoding myc-tagged human ferritin heavy chain (myc-hFTH) and green fluorescent protein (GFP), abbreviated as Lenti-myc-hFTH, was constructed by Kim et al. for use in cell tracking studies with magnetic resonance imaging (MRI) and optical imaging (1).

Gene reporters have recently been integrated into molecular imaging, and their ability to visualize transgene localization and expression in vivo has been changing the way of gene transfer studies (2, 3). This integration makes it possible to answer practical questions of a gene therapy paradigm in clinical settings (3). One of the typical reporters is the ferritin gene (4). Ferritin is a globular protein that consists of two subunits, heavy chain (FTH) and light chain (FTL). In both prokaryotes and eukaryotes, ferritin is the primary intracellular iron-storage protein that stores iron and releases it in a controlled fashion. All MRI studies with the ferritin gene have demonstrated its feasibility as a reliable transgene reporter (1, 4, 5). Forced expression of ferritin in cells after ferritin gene transfection is sufficient to augment cellular iron uptake to a degree detectable with MRI (2, 6). For example, Cohen et al. transfected the murine FTH gene into C6 glioma cells, and the induced expression of murine FTH led to decreased T2 relaxation times (7). Genove et al. introduced both FTH and FTL genes into mouse brain tissues, which enabled visualization of the transgene expression in mouse brain tissues with MRI (6). Deans et al. described the possibility to improve cellular contrast with a combined reporter system of transferrin receptor and ferritin (8). Furthermore, evidence indicates that ferritin overexpression does not interfere with the viability, proliferation, and differentiation of transfected cells (1, 9).

Both viral and non-viral approaches for introducing reporter genes into cells or tissues of interest have been investigated (1, 2, 10). Viral vectors such as retrovirus and adenovirus achieve highly efficient gene delivery into the target tissues, but their usefulness in humans is limited by issues of immunogenicity, random insertion into the host genome and potential mutagenesis, uncontrollable chronic expression of the gene, risk of systemic spread of the virus, and limited size of the inserted gene. Non-viral delivery approaches, such as lipofection, electroporation, ultrasound, and gene gun, are generally safe and simple, but they exhibit much lower transfection efficiency than viral vectors (2, 10). Kim et al. have reported a lentiviral vector construct that expresses both recombinant myc-hFTH and GFP (Lenti-myc-hFTH) for simultaneous MRI and optical imaging (1). The HIV type 1–derived lentiviral vector exhibits efficient gene delivery and stable expression of transgenes for both mitotic and nonmitotic cells. In contrast to adenoviral vectors, lentiviral vector delivery systems do not induce humoral responses to injected viral antigens. However, similar to retroviral vectors, lentiviral vectors integrate into the host genome. Studies by Kim et al. have shown that the lentiviral construct–transfected cells accumulated more iron than mock-transfected controls, which produced a pronounced contrast in MRI (1). The Lenti-myc-hFTH system may be used to monitor tumor growth, metastasis, and regression during cell- and gene-based therapies in deep tissues (1).

### Related Resource Links:

- Chapters on cell tracking in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=cell+tracking+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Clinical trials for cell tracking in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=cell+tracking+and+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20823165)]

Kim et al. detailed the procedures for the construction of Lenti-myc-hFTH (1). The phosphoglycerate kinase promoter was inserted immediately upstream of GFP in the lentiviral vector (LentiM1.41). The recombinant myc-hFTH was inserted into the BamHI-EcoRI restriction site under the control of cytomegalovirus immediate-early promoter and puromycin-resistant gene. The cDNA sequence of the constructed lentiviral vector was confirmed with DNA sequencing. The lentiviral vector without GFP and hFTH insertions was used for control (mock) transfection. The viral vector particles were produced with 293T cells and titrated with p24 enzyme-linked immunosorbent assay or with HeLa cell infection. The GFP expression was imaged with fluorescent microscopy. In routine preparations, the unconcentrated titer of the viral particles in culture supernatant was ~10^6^–10^7^ transduction units/ml.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20823165)]

To generate stable cell lines expressing myc-hFTH and GFP, MCF-7 human breast cancer cells and F-98 rat glioma cells were transduced with the lentivirus supernatants for 6–10 h in the presence of 4–8 µg/ml polybrene (1). Transduced cells were selected with 1 µg/ml puromycin in the media for 3–4 weeks and were then sorted with a fluorescence-activated cell sorter. Clones that express high levels of myc-hFTH and GFP were passaged and maintained in the growth medium containing 1 µg/ml puromycin. The transfection efficiency for both MCF-7 and F-98 cells was >90% with the Lenti-myc-hFTH vector. The presence of myc-hFTH and GFP expression in transfected cells and their absence in the no-vector and mock controls were confirmed with immunofluorescence and Western blotting. No differences in the cell viability and growth were observed among cells transfected with Lenti-myc-hFTH, mock, or no-vector.

The iron accumulation abilities of the Lenti-myc-hFTH–, mock-, and no-vector–transfected cells were evaluated with Prussian blue staining and MRI after treatment with ferric ammonium citrate (FAC) (20–500 µmol/L) for 72 hours (1). Iron accumulation for all cells increased in a manner dependent on the FAC dose. The Lenti-myc-hFTH cells had more accumulation of intracellular iron than mock and no-vector cells as detected with Prussian blue staining. T2*-Weighted MRI (1.5 T) of the agarose phantom containing 1 × 10^7^ cells showed a dark signal that was easily discernable in the Lenti-myc-hFTH cells treated with FAC (300 µmol/L). The T2* relaxation times of mock and Lenti-myc-hFTH cells in the absence of FAC were 30.3 ± 0.65 ms and 26.01 ± 1.4.5 ms, respectively. The T2* relaxation times of mock and Lenti-myc-hFTH cells in the presence of FAC were significantly lower (P ≤ 0.05), 22.03 ± 1.14 ms and 18.3 ± 0.31 ms, respectively. The treatment with 100 µmol/L FAC caused higher mitochondrial polarization in no-vector and mockcells than in myc-hFTH cells. The treatment with FAC (20–500 µmol/L) for 72 hours did not cause cellular toxicity in Lenti-myc-hFTH cells, whereas the viability of no-vector and mock cells decreased after treatment with FAC (P < 0.05). The results imply that myc-hFTH gene expression is protective against FAC toxicity (1).

The MRI detection sensitivity was evaluated for the mock, Lenti-myc-hFTH, Lenti-myc-hFTH with FAC, and Feridex-labeled cells (1). Feridex is a clinically approved and commercially available superparamagnetic iron oxide contrast agent. Feridex-labeled cells were collected after 24 h of incubation with 12.5 µg Fe/ml Feridex. Significant signal decreases were detected for 2 × 10^3^ Lenti-myc-hFTH cells and Feridex-labeled cells compared with the same number of mock cells. The T2* relaxation times of 2 × 10^3^ mock, Lenti-myc-hFTH, Lenti-myc-hFTH with FAC, and Feridex-labeled cells were 444.4 ± 96.2 ms, 305.6 ± 48.1 ms, 277.8 ± 48.1 ms, and 169.8 ± 28.7 ms, respectively. The T2* relaxation times of 2 × 10^4^ mock, Lenti-mychFTH, Lenti-myc-hFTH with FAC, and Feridex-labeled cells were 444.4 ± 96.3 ms, 241.3 ± 103.8 ms, 188.9.8 ± 19.24.1 ms, and 144.8 ± 20.9 ms, respectively. The detection sensitivity of Feridex-labeled cells was greater than that of Lenti-myc-hFTH cells under the above conditions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20823165)]

MRI (1.5 T) and optical imaging were performed in nude mice (n = 2) and Fisher 344 rats (n = 9) bearing subcutaneous MCF-7 tumor xenografts (1). In the mouse model, optical imaging showed detectable GFP in the Lenti-myc-hFTH tumors, but not in the mock tumors, 21 days after cell transplantation. T2-Weighted images of the Lenti-myc-hFTH tumors revealed lower signals than images of the mock tumors.

In the rat tumor model, hypointense signal in the T2- and T2*-weighted images of Lenti-myc-hFTH tumors was detected. The T2* relaxation times of mock and Lenti-myc-hFTH tumors at 3 weeks after transplantation were ~63.3 ± 7.5 ms and 35.9 ± 6.1 ms, respectively. The signal intensity of Lenti-myc-hFTH tumor was significantly lower than the mock tumor (P < 0.05). The signal intensity of Lenti-myc-hFTH tumors decreased from 2 weeks to 4 weeks with a significant decrease (P < 0.05) at 3–4 weeks.

Western blotting and immunostaining of the tumor samples showed that the myc-hFTH and GFP proteins were expressed only in the Lenti-myc-hFTH tumors. The sites expressing myc-hFTH also expressed GFP. Prussian blue staining demonstrated large deposits of accumulated iron in the Lenti-myc-hFTH tumors at 3 weeks after transplantation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Kim H.S., Cho H.R., Choi S.H., Woo J.S., Moon W.K. (2010). In vivo imaging of tumor transduced with bimodal lentiviral vector encoding human ferritin and green fluorescent protein on a 1.5T clinical magnetic resonance scanner. Cancer Res.
2 Hasegawa S., Furukawa T., Saga T. (2010). Molecular MR imaging of cancer gene therapy: ferritin transgene reporter takes the stage. Magn Reson Med Sci.
3 Waerzeggers Y., Monfared P., Viel T., Winkeler A., Voges J., Jacobs A.H. (2009). Methods to monitor gene therapy with molecular imaging. Methods.
4 Cohen B., Ziv K., Plaks V., Harmelin A., Neeman M. (2009). Ferritin nanoparticles as magnetic resonance reporter gene. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
5 Hasegawa, S., S. Saito, J.I. Takanashi, Y. Morokoshi, T. Furukawa, T. Saga, and I. Aoki, Evaluation of ferritin-overexpressing brain in newly developed transgenic mice. Magn Reson Imaging, 2010
6 Genove G., DeMarco U., Xu H., Goins W.F., Ahrens E.T. (2005). A new transgene reporter for in vivo magnetic resonance imaging. Nat Med.
7 Cohen B., Dafni H., Meir G., Harmelin A., Neeman M. (2005). Ferritin as an endogenous MRI reporter for noninvasive imaging of gene expression in C6 glioma tumors. Neoplasia.
8 Deans A.E., Wadghiri Y.Z., Bernas L.M., Yu X., Rutt B.K., Turnbull D.H. (2006). Cellular MRI contrast via coexpression of transferrin receptor and ferritin. Magn Reson Med.
9 Naumova A.V., Reinecke H., Yarnykh V., Deem J., Yuan C., Murry C.E. (2010). Ferritin overexpression for noninvasive magnetic resonance imaging-based tracking of stem cells transplanted into the heart. Mol Imaging.
10 Gilad A.A., Winnard P.T., van Zijl P.C., Bulte J.W. (2007). Developing MR reporter genes: promises and pitfalls. NMR Biomed.